# ^18^F-Labeled N-(4-fluorobenzylidene)oxime-monomeric Z_HER2:477_

Chemical name: | ^18^F-N-(4-fluorobenzylidene)oxime-monomeric Z_HER2:477_ | [image]
Abbreviated name: | ^18^F-FBO-Z_HER2:477_ | [image]
Synonym: | | [image]
Agent Category: | Affibody, antibody | [image]
Target: | HER2 | [image]
Target Category: | Receptor | [image]
Method of detection: | Positron emission tomography (PET) | [image]
Source of signal / contrast: | ^18^F | [image]
Activation: | No | [image]
Studies: | - In vitro; - Rodents | Structure of the agents by Cheng et al. (1).

## Background

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=affibody%20and%20HER2%20and%20molecular%20imaging)]

The ^18^F-labeled N-(4-fluorobenzylidene)oxime (FBO)-monomeric Z_HER2:477_ conjugate, abbreviated as ^18^F-FBO-Z_HER2:477_, is an affibody derivative synthesized by Cheng et al. for positron emission tomography (PET) of HER2-expressing tumors (1).

Affibody molecules are a group of nonimmunogenic scaffold proteins that derive from the B-domain of staphylococcal surface protein A (2, 3). In the past several years, affibodies have drawn significant attention for developing imaging and therapeutic agents because of their unique features (3, 4). First, affibodies are small, with only 58 amino acid residues (~7 kDa) (3, 5). The small size allows affibodies to be generated with solid-phase peptide synthesis and to be cleared quickly by the kidneys. Second, affibodies have a high binding affinity and specificity to their targets. Their binding affinity can be further improved by generating multimeric constructs through the solvent-exposed termini of affibody Z-domain. The anti-HER2 monomeric affibody Z_HER2:4_ is an example that has a binding affinity of ~50 nM, but its dimeric form, (Z_HER2:4_)_2_, exhibits an improved binding affinity of up to ~3 nM (6). Third, affibodies lack cysteine residues and disulfide bridges in structure, and they fold rapidly. These features make it possible to chemically synthesize fully functional molecules and to introduce unique cysteine residues or chemical groups into affibodies for site-specific labeling. Several anti-HER2 affibody derivatives have been synthesized in this way. The imaging agent HPEM-His_6_-(Z_HER2:4_)_2_-Cys was generated by radiobrominating the dimeric (Z_HER2:4_)_2_ through the cysteine residues that were introduced to the C-terminus of (Z_HER2:4_)_2_ (7). Several affibody derivatives (e.g., ^68^Ga-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK48901/), ^111^In-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK23176/), ^111^In-benzyl-DOTA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23058/), and ^111^In-benzyl-DTPA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23322/)) were synthesized by coupling a chelating agent with a specifically protected site group of the Z_HER2:342_ peptide chain (3). Furthermore, these small affibody proteins can be selected and optimized with a strategy of sequence mutation and affinity maturation, and an example selected with this strategy is the anti-HER2 affibody Z_HER2:342_, which has an increased affinity of 50 nM (Z_HER2:4_, the first generation) to 22 pM (8).

The investigators at Stanford University first tested the feasibility of the monomeric and dimeric forms of anti-HER2 affibody Z_HER2:477_ for molecular imaging. Both forms of the Z_HER2:477_ molecule were radiofluorinated with an ^18^F-labeled prosthetic group of 4-^18^F-fluorobenzaldehyde (^18^F-FBO-Z_HER2:477_ and ^18^F-FBO-(Z_HER2:477_)_2_, respectively) (1). The investigators have also coupled ^64^Cu to the affibody through DOTA, leading to the development of imaging agents ^64^Cu-DOTA- Z_HER2:477_ and ^64^Cu-DOTA-(Z_HER2:477_)_2_ (9). Interestingly, these studies showed that smaller affibody constructs performed better in vivo in terms of tumor uptake and clearance in spite of the lower affinity in vitro. The investigators then generated a class of small proteins consisting of two α-helix bundles of the 3-helix affibody by deleting the helix 3 because the binding domain localizes in the α-helices 1 and 2 bundles (5). One of these 2-helix proteins is MUT-DS, which has α-helices 1 and 2 bundles, with a disulfide bridge being formed between the two inserted homocysteines (10-12). MUT-DS showed a binding affinity to HER2 in the low-nM range. The radiolabeled MUT-DS derivatives exhibited favorable pharmacokinetics for both imaging and therapy of HER2-expressing tumors (refer to MUT-DS derived agents in MICAD).

This series of chapters summarizes the data obtained with the Z_HER2:477_ derivatives, and this chapter presents the data obtained with ^18^F-FBO-Z_HER2:477_ (1).

### Related Resource Links:

- Anti-HER2 affibody conjugates in MICAD:

^68^Ga-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK48901/), ^111^In-DOTA-Z_HER2:342-pep2_ (http://www.ncbi.nlm.nih.gov/books/NBK23176/), Alexa750-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK45127/), ^111^In-benzyl-DOTA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23058/), ^111^In-benzyl-DTPA-Z_HER2:342_ (http://www.ncbi.nlm.nih.gov/books/NBK23322/), Eaff800 (http://www.ncbi.nlm.nih.gov/books/NBK45665/), DY-682-ABD-Z_HER2:342_ (Haff682) (http://www.ncbi.nlm.nih.gov/books/NBK45664/), ^99m^Tc-Z_2395_-C (http://www.ncbi.nlm.nih.gov/books/NBK23590/), [^111^In]-ABY-025 (http://www.ncbi.nlm.nih.gov/books/NBK45623/), ^111^In-BZ-DTPA-Z_EGFR:1907_ (http://www.ncbi.nlm.nih.gov/books/NBK23654/)

- HER2-related clinical trials for imaging and therapy (http://clinicaltrials.gov/ct2/results?term=HER2)

## Synthesis

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/18413392)]

The monomeric affibody Z_HER2:477_ with a distal C-terminal cysteine residue (purity, >95%) is commercially available. The agent ^18^F-FBO-Z_HER2:477_ was synthesized in three steps (1). The bifunctional linker 2-(aminooxy)-N-(2-(2,5-dioxo-2,5-dihydro-^1^H-pyrrol-1-yl)ethyl)acetamide hydrochloride was first prepared by reacting N-(2-aminoethyl)malemide with 2-(tert-butoxycarbonylaminooxy)acetic acid under carbodiimide-mediated coupling conditions. The linker consisted of two orthogonal groups, a thiol-reactive maleimide group for conjugation to the cysteine residue and an ^18/19^F-aldehyde–reactive aminooxy group. The yield was 80%. The linker was then selectively conjugated to the affibody molecule to generate aminooxy-functionalized Z_HER2:477_ (Z_HER2:477_-ONH_2_; yield = 82%; molecular weight (MW) = 6,962.58 Da). As the last step, Z_HER2:477_-ONH_2_ was conjugated with 4-fluorobenzaldehyde (4-FBA), which resulted in the nonradioactive FBO-Z_HER2:477_. The recovery yield was 70%–90%, and the measured MW was 7,068.94 Da for the nonradioactive FBO-Z_HER2:477_. Similarly, conjugation of the Z_HER2:477_-ONH_2_ with 4-^18^F-FBA led to the generation of radioactive ^18^F-FBO-Z_HER2:477_. For radiolabeling, the coupling yield was 30%–40%, and the overall radiochemical yield ranged from 13% to 18% (end of synthesis, corrected for decay). The specific activity and purity of ^18^F-FBO-Z_HER2:477_ were 13.0–20.7 MBq/nmol (50–80 μCi/μg) and >95%, respectively, at end of synthesis. The total synthesis time was ~100 min.

## In Vitro Studies: Testing in Cells and Tissues

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/18413392)]

Binding affinity with the extracellular domain of HER2 antigen was measured in vitro with surface plasmon resonance detection (1). The measurements showed that the binding affinities of Z_HER2:477_-ONH_2_ and FBO-Z_HER2:477_ were 400 and 430 pM, respectively (180 and 200 pM for the dimeric forms (Z_HER2:477_)_2_-ONH_2_ and FBO-(Z_HER2:477_)_2_, respectively). The association constants were in the range of 10^5^–10^6^ (association time, >2 min), and the dissociation constants were in the range of 10^-4^–10^-5^ (disassociation time, >15 min), indicating that the on rate was very fast and the off rate was very slow.

The HER2-targeting ability for cultured cells was evaluated with SKOV3 human ovarian cancer cells (0.2 × 10^6^ cells/well) after incubation for 2 h with 1.11−6.29 kBq (0.03–0.17 μCi) ^18^F-FBO-Z_HER2:477_. ^18^F-FBO-Z_HER2:477_ quickly accumulated in the SKOV3 cells and reached the value of 0.00476 cell counts per minute [cpm]/medium cpm/μg of protein/μL at 0.5 h, which was maintained up to 2 h. In the presence of a large excess of nonradioactive Z_HER2:477_ (final concentration, 0.28 μM), the cell uptake of ^18^F-FBO-Z_HER2:477_ was inhibited significantly at all incubation time points (P < 0.05), showing a value of only 0.00329 from the unblocked amount of 0.00476 at 0.5 h, which suggests that the agent is specific to HER2 (1).

## Animal Studies

### Rodents

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/18413392)]

Biodistribution studies were performed in nude mice bearing SKOV3 tumors (n = 3 mice/time point) (1). Mice were injected via the tail vein with 0.37–1.11 MBq (10–30 μCi) ^18^F-FBO-Z_HER2:477_ and then euthanized at different time points after injection. The radioactivity in ex vivo tissues was expressed as a percentage of the injected radioactive dose per gram of tissue (% ID/g). Rapid and high accumulation of ^18^F-FBO-Z_HER2:477_ in SKOV3 tumors was observed at early time points (4.77 ± 0.78% ID/g at 0.5 h after injection), and accumulation decreased to 3.61 ± 0.29% ID/g at 3 h after injection. At 3 h after injection, the tumor/blood and tumor/muscle ratios were 12.72 ± 2.94 and 28.03 ± 8.28, respectively.

Compared to the dimeric form (refer to the chapter of ^18^F-FBO-(Z_HER2:477_)_2_ in MICAD), ^18^F-FBO-Z_HER2:477_ showed significantly higher tumor/normal tissue (blood, muscle, liver, and lung) ratios at all time points. Both monomeric and dimeric forms displayed relatively rapid blood clearance, with blood uptake values of 3.81 ± 0.50% and 1.97 ± 0.24% ID/g at 0.5 h (P < 0.05), respectively, and 1.50 ± 0.35% and 1.56 ± 0.29% ID/g at 1 h after injection, respectively. In the kidneys, both forms displayed very high levels of uptake, especially at the early time points (>20% ID/g at 0.5 h after injection), and the monomeric form had a comparatively higher renal uptake than the dimeric form. On the contrary, the dimeric form showed significantly higher levels of uptake in the liver and muscle at 0.5 h after injection than the monomeric form, but both forms displayed similar levels of uptake at later time points.

PET imaging was performed in mice bearing SKOV3 tumors at 0.5, 1, 2, and 4 h after tail vein injection of ^18^F-FBO-Z_HER2:477_ (0.444–0.814 MBq (12–22 μCi)) or ^18^F-FBO-(Z_HER2:477_)_2_ (1.85–2.035 MBq (50–55 μCi)) (1). The tumor was visible with both forms, especially at later time points, but a better tumor/background contrast was observed with the monomeric form. ^18^F-FBO-Z_HER2:477_ had approximately two-fold higher tumor uptake than ^18^F-FBO-(Z_HER2:477_)_2_. High levels of activity accumulation were observed in the kidneys and the intestinal tract for both forms.

To test the in vivo HER2-targeting specificity of ^18^F-FBO-Z_HER2_, nude mice bearing SKOV3 tumors (n = 3 mice/each group) were pretreated with either 500 μg trastuzumab or 300 μg affibody Z_HER2:477_ (1). Mice were then given ^18^F-FBO-Z_HER2:477_ at 72 h after trastuzumab injection and at 1 h after Z_HER2:477_ injection. Mice without pretreatment were used as a control. The biodistribution at 1 h after ^18^F-FBO-Z_HER2:477_ injection was examined. Pretreatment with Z_HER2:477_ specifically reduced the tumor uptake of ^18^F-FBO-Z_HER2:477_ (1.73 ± 0.37% ID/g) to ~36% of the control tumor uptake (4.77 ± 0.88%; P < 0.05). No significant difference was observed for the uptake in normal tissues. Pretreatment with trastuzumab specifically inhibited the uptake of ^18^F-FBO-Z_HER2:477_ (2.25 ± 0.49% ID/g) to ~47% of the control tumor uptake (4.77 ± 0.88%; P < 0.05), and again no inhibition of the uptake was observed in normal organs.

In conclusion, studies by Cheng et al. showed that ^18^F-FBO-Z_HER2:477_ rapidly localized in SKOV3 tumors and exhibited good tumor uptake, retention, tumor/muscle ratio, and high specificity to HER2 (1). Compared to its dimeric form, ^18^F-FBO-Z_HER2:477_ showed better in vivo performance, although it had a lower affinity with HER2 and a lower cell uptake in vitro. ^18^F-FBO-Z_HER2:477_ is more promising than its dimeric form as an agent for HER2 imaging (1).

### Other Non-Primate Mammals

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28dog%20OR%20rabbit%20OR%20pig%20OR%20sheep%29)]

No references are available.

### Non-Human Primates

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20%28primate%20NOT%20human%29)]

No references are available.

## Human Studies

[PubMed (http://www.ncbi.nlm.nih.gov/pubmed/?term=%22SUBSTANCENAME%22%5BSubstance%20Name%5D%20AND%20human)]

No references are available.

## References

1 Cheng Z., De Jesus O.P., Namavari M., De A., Levi J., Webster J.M., Zhang R., Lee B., Syud F.A., Gambhir S.S. (2008). Small-animal PET imaging of human epidermal growth factor receptor type 2 expression with site-specific 18F-labeled protein scaffold molecules. J Nucl Med.
2 Friedman M., Nordberg E., Hoiden-Guthenberg I., Brismar H., Adams G.P., Nilsson F.Y., Carlsson J., Stahl S. (2007). Phage display selection of Affibody molecules with specific binding to the extracellular domain of the epidermal growth factor receptor. Protein Eng Des Sel.
3 Orlova A., Feldwisch J., Abrahmsen L., Tolmachev V. (2007). Update: affibody molecules for molecular imaging and therapy for cancer. Cancer Biother Radiopharm.
4 Tolmachev V., Orlova A., Nilsson F.Y., Feldwisch J., Wennborg A., Abrahmsen L. (2007). Affibody molecules: potential for in vivo imaging of molecular targets for cancer therapy. Expert Opin Biol Ther.
5 Webster J.M., Zhang R., Gambhir S.S., Cheng Z., Syud F.A. (2009). Engineered two-helix small proteins for molecular recognition. Chembiochem.
6 Steffen A.C., Wikman M., Tolmachev V., Adams G.P., Nilsson F.Y., Stahl S., Carlsson J. (2005). In vitro characterization of a bivalent anti-HER-2 affibody with potential for radionuclide-based diagnostics. Cancer Biother Radiopharm.
7 Mume E., Orlova A., Larsson B., Nilsson A.S., Nilsson F.Y., Sjoberg S., Tolmachev V. (2005). Evaluation of ((4-hydroxyphenyl)ethyl)maleimide for site-specific radiobromination of anti-HER2 affibody. Bioconjug Chem.
8 Orlova A., Magnusson M., Eriksson T.L., Nilsson M., Larsson B., Hoiden-Guthenberg I., Widstrom C., Carlsson J., Tolmachev V., Stahl S., Nilsson F.Y. (2006). Tumor imaging using a picomolar affinity HER2 binding affibody molecule. Cancer Res.
9 Cheng Z., De Jesus O.P., Kramer D.J., De A., Webster J.M., Gheysens O., Levi J., Namavari M., Wang S., Park J.M., Zhang R., Liu H., Lee B., Syud F.A., Gambhir S.S. (2010). 64Cu-labeled affibody molecules for imaging of HER2 expressing tumors. Mol Imaging Biol.
10 Ren, G., J.M. Webster, Z. Liu, R. Zhang, Z. Miao, H. Liu, S.S. Gambhir, F.A. Syud, and Z. Cheng, In vivo targeting of HER2-positive tumor using 2-helix affibody molecules. Amino Acids, 2011
11 Ren G., Zhang R., Liu Z., Webster J.M., Miao Z., Gambhir S.S., Syud F.A., Cheng Z. (2009). A 2-helix small protein labeled with 68Ga for PET imaging of HER2 expression. J Nucl Med.
12 Miao Z., Ren G., Jiang L., Liu H., Webster J.M., Zhang R., Namavari M., Gambhir S.S., Syud F., Cheng Z. (2011). A novel (18)F-labeled two-helix scaffold protein for PET imaging of HER2-positive tumor. Eur J Nucl Med Mol Imaging.